# ^99m^Tc-Labeled 6-hydrazinopyridine-3-carboxylic acid (HYNIC)–conjugated murine anti-MUC1 monoclonal antibody PR81

Chemical name: | ^99m^Tc-Labeled 6-hydrazinopyridine-3-carboxylic acid (HYNIC)–conjugated murine anti-MUC1 monoclonal antibody PR81
Abbreviated name: | [^99m^Tc]-PR81
Synonym:
Agent Category: | Antibody
Target: | Mucin (human epithelial)
Target Category: | Antigen
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=MUC1%20glycoprotein&cmd=DetailsSearch)]

Mucins, such as MUC1, belong to a large group of highly glycosylated transmembrane proteins that are expressed on the surface of most epithelial cells and to a smaller extent on T- and B-lymphocytes, nerve cells, monocytes, and hepatocytes (1). The structure and functions of these glycoproteins have been discussed in detail by Hattrup and Gendler (2). Upregulated gene expression and under-glycosylation of MUC1 have been reported in different cancers, particularly that of the breast, and usually indicate a poor prognosis for the patient (3, 4). Therefore, anti-MUC1 antibodies (Abs) have been used by several investigators to target this glycoprotein for the imaging and treatment of cancers with high expression of MUC1 (5, 6). Recently, a humanized anti-MUC1 Ab, AS1402, was studied to determine its safety, pharmacokinetic characteristics, and maximum tolerated dose in individuals with advanced breast cancer (4). From this study the investigators concluded that the Ab was well tolerated, and 5 of 26 patients showed stable disease lasting from 80 to 119 days, indicating that further investigation of the immunotherapy was necessary.

Recently, an anti-MUC1 monoclonal Ab (mAb), PR81, was developed from human breast cancer cell extracts and evaluated for possible use as an immuniscintigraphic agent for the detection of breast cancer (7). After labeling with ^99m^Tc, the biodistribution and scintigraphic properties of the labeled mAb ([^99m^Tc]-PR81) were investigated in mice bearing MCF-7 xenograft tumors (of human breast cancer origin and expressing high levels of MUC1).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=anti-MUC1%20PR81%20synthesis&cmd=DetailsSearch)]

The characteristics, production, and ^99m^Tc labeling of PR81 was described by Salouti et al. (7). The efficiency of the radiolabeling reaction was reported to be 89.2 ± 4.4% as determined with instant thin-layer chromatography (ITLC) using 0.9% saline as the running buffer (under these running conditions [^99m^Tc]-PR81remained at the origin). The final product contained 3.4 ± 0.9% radiocolloids as revealed with cellulose nitrate electrophoresis. The specific activity of ^99m^Tc-PR81 was ~740 MBq/mg (20 mCi/mg).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=anti-MUC1%20PR81%20in%20vitro%20studies&cmd=DetailsSearch)]

The in vitro stability of ^99m^Tc-PR81was 88.3 ± 4.6% (determine with ITLC) in phosphate-buffered saline (pH 7.4) when stored at room temperature for up to 24 h after labeling (7). The radiolabeled mAb was reported to have a stability of 79.8 ± 5.7% after exposure to human serum for 24 h at 37°C as determined with size-exclusion chromatography (7).

The binding of ^99m^Tc-PR81 to MCF-7 cells was studied with increasing concentrations of unlabeled PR81 in the assay medium (7). The cell binding of the labeled mAb was shown to be reduced from 30% of total radioactivity in presence of 1 μg PR81 to <1.0% with 1 mg PR81. From these results the investigators concluded that ^99m^Tc-PR81 had a high binding specificity for MUC1, which was similar to the native, unlabeled mAb.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=anti-MUC1%20PR81%20rodentia&cmd=DetailsSearch)]

The biodistribution of ^99m^Tc-PR81 was studied in Balb/c mice bearing MCF-7 cell tumors (7). The labeled mAb was administered to the mice by intravenous injection through the tail vein, and the animals (n = 5 mice/time point) were euthanized at predetermined time points ranging from 4 h to 24 h postinjection (p.i.). All major organs, including the tumors, were harvested from the euthanized animals, and the amount of accumulated radioactivity in the tissues was determined. Data from this study were presented as percent injected dose per gram tissue (% ID/g). At 4 h p.i., maximum radioactivity was observed in the large intestine (6.2 ± 0.8% ID/g), followed by the kidney (8.1 ± 3.7% ID/g), liver (6.4 ± 1.1% ID/g), and tumor (4.7 ± 2.4% ID/g). All other organs accumulated radioactivity between 1% and 4% ID/g radioactivity at this time point. At 16 h p.i., maximum radioactivity was reported in the large intestine (17.5± 5.9% ID/g), followed by the kidney (9.5 ± 1.9% ID/g), liver (5.3 ± 0.7% ID/g), and tumor (3.8 ± 0.7% ID/g). By 24 h p.i., the tumors had an accumulation of 4.3 ± 0.5% ID/g compared to 4.0 ± 0.4, 3.3 ± 0.5, and 1.2 ± 0.2% ID/g in the kidneys, liver, and large intestine, respectively. All other organs had between 0.2% and 2.0% ID/g radioactivity at this time point. From this study it was clear that radioactivity remained relatively constant in the tumors for up to 24 h. No blocking studies were reported.

Anterior and posterior whole-body radioimmunoscintigraphy was performed on ketamine-anesthetized mice at various time points for up to 36 h p.i (7). The tumors were clearly visible in the images at 8 h p.i. for up to 20 h however the image intensity was reported to be somewhat reduced beyond the 20 h time point. No blocking studies were reported.

From these studies, the investigators concluded that ^99m^Tc-PR81was suitable for the detection of human breast cancer xenograft tumors in mice (7). However, further evaluation of the labeled mAb is necessary before it can be used as a detection tool for breast cancer in humans.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=anti-MUC1%20PR81%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=anti-MUC1%20PR81%20Non-Human%20Primates&cmd=DetailsSearch)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=anti-MUC1%20PR81%20Human%20Studies&cmd=DetailsSearch)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No supplemental information is currently available.

## References

1 Zaretsky J.Z., Barnea I., Aylon Y., Gorivodsky M., Wreschner D.H., Keydar I. (2006). MUC1 gene overexpressed in breast cancer: structure and transcriptional activity of the MUC1 promoter and role of estrogen receptor alpha (ERalpha) in regulation of the MUC1 gene expression. Mol Cancer.
2 Hattrup C.L., Gendler S.J. (2008). Structure and function of the cell surface (tethered) mucins. Annu Rev Physiol.
3 Yuan Z., Wong S., Borrelli A., Chung M.A. (2007). Down-regulation of MUC1 in cancer cells inhibits cell migration by promoting E-cadherin/catenin complex formation. Biochem Biophys Res Commun.
4 Pegram M.D., Borges V.F., Ibrahim N., Fuloria J., Shapiro C., Perez S., Wang K., Schaedli Stark F., Courtenay Luck N. (2009). Phase I dose escalation pharmacokinetic assessment of intravenous humanized anti-MUC1 antibody AS1402 in patients with advanced breast cancer. Breast Cancer Res.
5 Singh R., Bandyopadhyay D. (2007). MUC1: a target molecule for cancer therapy. Cancer Biol Ther.
6 Albrecht H., Denardo G.L., Denardo S.J. (2007). Development of anti-MUC1 di-scFvs for molecular targeting of epithelial cancers, such as breast and prostate cancers. Q J Nucl Med Mol Imaging.
7 Salouti M., Rajabi H., Babaei M.H., Rasaee M.J. (2008). Breast tumor targeting with (99m)Tc-HYNIC-PR81 complex as a new biologic radiopharmaceutical. Nucl Med Biol.